# ^99m^Tc-Labeled 1-hydroxy-3-(1H-imidazol-1-yl)propane-1,1-diyldiphosphonic acid (IPrDP)

Chemical name: | ^99m^Tc-Labeled 1-hydroxy-3-(1H-imidazol-1-yl)propane-1,1-diyldiphosphonic acid (IPrDP)
Abbreviated name: | [^99m^Tc]-IPrDP
Synonym:
Agent Category: | Compound
Target: | Bone (hydroxyapatite); farnesyl disphosphate (pyrophosphate) synthase (molecular target)
Target Category: | Tissue; enzyme
Method of detection: | Single-photon emission tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals | Click on the Click on the above proposed structure of [^99m^Tc]-IPrDP (1) for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Bisphosphonates&cmd=DetailsSearch)]

Bisphosphonates (BPs; also known as idphosphonates) labeled with technetium ([^99m^Tc]-BP) are often used with bone scintigraphy to detect osteoporosis and other skeletal-related events (SREs), including bone metastases (2). These chemicals are known to promote osteoclast apoptosis and have a strong affinity for hydroxyapatite, a component of the bone matrix. The mechanism of action of these bone-seeking compounds is described in detail elsewhere (3-5). Bone scintigraphy is usually performed 2–6 h after intravenous injection of a [^99m^Tc]-BP, resulting in exposure of the patient to radiation for an extended time. To develop BPs that are more efficient and require only a short waiting time before bone scintigraphy, investigators generated various BPs, such as zoledronic acid (http://www.pharma.us.novartis.com/product/pi/pdf/Zometa.pdf) (ZL), which contains an imidazole group in its structure, and evaluated their efficacy for the treatment of various bone-related diseases (6, 7). ZL was determined to be the most potent BP available for treating bone resorption and is approved by the United States Food and Drug Administration for the treatment of various tumor-induced SREs (8).

In an earlier study with a goal to further improve the potency of ZL, the imidazole group of the compound was modified to obtain 1-hydroxy-2-(2-ethyl-4-methyl-1H-imidazol-1-yl)ethane-1,1-diyldiphosphonic acid (EMIDP), and the chemical was labeled with ^99m^Tc to produce [^99m^Tc]-EMIDP (2). The biodistribution of [^99m^Tc]-EMIDP was investigated in normal mice, and the radiochemical was evaluated as a bone-imaging agent in rabbits. From these studies, the investigators concluded that [^99m^Tc]-EMIDP bound selectively to the skeletal tissue in rabbits, which is superior to the selectivity of ^99m^Tc-labeled methylene diphosphonate ([^99m^Tc]-MDP), another BP that is commonly used in the clinic. In a continued effort to explore the possibility of generating a high-potency ZL derivative similar to EMIDP, Lin et al. investigated optimization of the linker chain between the imidazolyl and the germinal BP group in the structure of ZL (1). For this, a ZL derivative, 1-hydroxy-3-(1H-imidazol-1-yl)propane-1,1-diyldiphosphonic acid (IPrDP) was synthesized, labeled with ^99m^Tc (to obtain [^99m^Tc]-IPrDP), and investigated for its biodistribution in normal mice. In addition, the bone-imaging properties of [^99m^Tc]-IPrDP with single-photon emission computed tomography (SPECT) imaging were compared with those of [^99m^Tc]-ZL in rabbits.

### Related Resource Links

Related chapters (http://www.ncbi.nlm.nih.gov/books/?term=MDP+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books) in MICAD

Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/NM_001037277.1) of human farnesyl diphosphate synthase

Gene information (http://www.ncbi.nlm.nih.gov/gene/2224) regarding human farnesyl diphosphate synthase (GeneID: 2224)

Farnesyl diphosphate synthase in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/omim/134629)

Structure of farnesyl diphosphate synthase (http://www.ncbi.nlm.nih.gov/Structure/mmdb/mmdbsrv.cgi?uid=59201) complexed with a bisphosphonate

Farnesyl diphosphate synthase in Kyoto Encyclopedia of Genes and Genomes (KEGG) Pathways (http://www.genome.jp/dbget-bin/www_bget?pathway+hsa00900)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=bisphosphonates) with bisphosphonates (or diphosphonates)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-IPrDP%20synthesis&cmd=DetailsSearch)]

The synthesis and labeling of IPrDP with ^99m^ Tc has been described by Lin et al. (1). Both the radiochemical purity and radiochemical yield of [^99m^Tc]-IPrDP were reported to be 97.2%, as determined with thin-layer chromatography. The specific activity (n = 3 determinations) of the radiochemical was 185 ± 17 MBq/nmol (5 ± 0.46 mCi/nmol).

For use as a control, [^99m^Tc]-ZL was also prepared with the same method as described for the production of [^99m^Tc]-IPrDP (1). The radiochemical purity, radiochemical yield, and specific activity of [^99m^Tc]-ZL were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-IPrDP%20in%20vitro&cmd=DetailsSearch)]

The in vitro stability of [^99m^Tc]-IPrDP was determined by measuring the radiochemical purity of the radiolabeled compound after incubating a fresh preparation of the tracer (buffer not described) for up to 6 h at room temperature (1). The labeled chemical was reported to maintain a radiochemical purity of >95% for at least 6 h at room temperature.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-IPrDP%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^99m^Tc]-IPrDP (1.85 MBq (0.05 mCi)) was studied in normal Institute of Cancer Research mice (1). The animals (n = 5 mice/group) were injected with the radioligand through the tail vein and euthanized at predetermined time points ranging from 5 min postinjection (p.i.) to 240 min p.i. to determine the amount of radioactivity accumulated in all the major organs, including bone. Data obtained from this study was expressed as a percent of injected dose per gram tissue (% ID/g).

A control set of mice (n = 5 animals/group) were injected with [^99m^Tc]-ZL (1.85 MBq (0.05 mCi)) and treated as described above.

With [^99m^Tc]-IPrDP, the amount of radioactivity accumulated in the bone was 5.37 ± 0.36% ID/g at 5 min p.i., peaked at 11.14 ± 1.85% ID/g at 60 min p.i., and decreased to 8.46 ± 0.44 at 240 min p.i. With [^99m^Tc]-ZL, uptake in the bone was 3.19 ± 0.45% ID/g at 5 min p.i., peaked at 11.7 ± 1.54% ID/g at 120 min p.i., and decreased to 9.95 ± 0.43% ID/g at 240 min p.i. The accumulation of radiolabel in the liver with [^99m^Tc]-IPrDP increased from ~3.5% ID/g to ~5.5% ID/g from 5 min p.i. to 240 min p.i., whereas with [^99m^Tc]-ZL the uptake was >30% ID/g at all the time points. A similar trend was observed in the spleen (<4% ID/g for [^99m^Tc]-IPrDP and >15% ID/g with [^99m^Tc]-ZL at all time points). In the kidney, the uptake of radioactivity from [^99m^Tc]-IPrDP decreased from 13.80 ± 1.34% ID/g at 5 min p.i. to 4.54 ± 0.26% ID/g at 240 min p.i., and with [^99m^Tc]-ZL the amount of accumulated tracer decreased from 13.10 ± 0.74% ID/g to 2.13 ± 0.47% ID/g during the same period. The bone/blood ratio with [^99m^Tc]-IPrDP increased from 0.76 at 5 min p.i. to 16.1 at 60 min p.i., but with [^99m^Tc]-ZL this ratio was ~1 and ~3.3 at 5 min p.i. and 60 min p.i., respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-IPrDP%20Non-Primate%20Mammals&cmd=DetailsSearch)]

The bone-imaging properties of [^99m^Tc]-IPrDP were investigated in rabbits (n = 1 animal/tracer) and compared with those of [^99m^Tc]-ZL in the same animals (1). The rabbits were anesthetized with a mixture of 0.2 g ketamine and 10 mg diazepam and injected with either [^99m^Tc]-IPrDP or [^99m^Tc]-ZL (155 MBq (4.2 mCi)) through the marginal ear vein; the mice were then scanned to acquire SPECT images at various time points. From the images, it was clear that both radiocompounds accumulated mainly in the skeleton, kidneys, and the urinary bladder of the animals. The rabbit skeleton was clearly visible with [^99m^Tc]-IPrDP at 1 h p.i., indicating a selective binding of the tracer to the bone and rapid clearance from the soft tissues as observed during the biodistribution studies with mice (see above). The bone/soft tissue uptake (B/T) ratios were calculated from the various images as detailed by Lin et al. (1). The B/T ratios with [^99m^Tc]-IPrDP were observed to be higher than those of [^99m^Tc]-ZL at all time points. This indicated that, compared to [^99m^Tc]-ZL, the radioactivity from [^99m^Tc]-IPrDP was rapidly cleared from the soft tissue of these animals.

In another study, rabbits were injected with [^99m^Tc]-IPrDP, [^99m^Tc]-ZL, and [^99m^Tc]-MDP (n = 1 animal/tracer), and static images were acquired from the animals at different time points ranging from 1 h p.i. to 4 h p.i (1). From the images, it was evident that the skeletal profile of the animals generated with [^99m^Tc]-IPrDP was superior to skeletal profiles obtained with either [^99m^Tc]-ZL or [^99m^Tc]-MDP from 2 h p.i. onward.

From these studies, the investigators concluded that [^99m^Tc]-IPrDP had superior biodistribution (in mice) and bone-imaging properties (in rabbits) compared to either [^99m^Tc]-ZL or [^99m^Tc]-MDP (1).

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-IPrDP%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-IPrDP%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Lin J., Qiu L., Cheng W., Luo S., Ye W. (2011). Preparation and in vivo biological investigations on a novel radioligand for bone scanning: technetium-99m-labeled zoledronic acid derivative. Nucl Med Biol.
2 Lin J., Luo S., Chen C., Qiu L., Wang Y., Cheng W., Ye W., Xia Y. (2010). Preparation and preclinical pharmacological study on a novel bone imaging agent (99m)Tc-EMIDP. Appl Radiat Isot.
3 Kimmel D.B. (2007). Mechanism of action, pharmacokinetic and pharmacodynamic profile, and clinical applications of nitrogen-containing bisphosphonates. J Dent Res.
4 Zhang Y., Cao R., Yin F., Hudock M.P., Guo R.T., Krysiak K., Mukherjee S., Gao Y.G., Robinson H., Song Y., No J.H., Bergan K., Leon A., Cass L., Goddard A., Chang T.K., Lin F.Y., Van Beek E., Papapoulos S., Wang A.H., Kubo T., Ochi M., Mukkamala D., Oldfield E. (2009). Lipophilic bisphosphonates as dual farnesyl/geranylgeranyl diphosphate synthase inhibitors: an X-ray and NMR investigation. J Am Chem Soc.
5 Mitterhauser M., Toegel S. (2011). Radiopharmaceutical considerations on bone seeker uptake: should we learn from therapeutical targets of bisphosphonates?. Nucl Med Biol.
6 Widler L., Jaeggi K.A., Glatt M., Muller K., Bachmann R., Bisping M., Born A.R., Cortesi R., Guiglia G., Jeker H., Klein R., Ramseier U., Schmid J., Schreiber G., Seltenmeyer Y., Green J.R. (2002). Highly potent geminal bisphosphonates. From pamidronate disodium (Aredia) to zoledronic acid (Zometa). J Med Chem.
7 Asikoglu M., Durak F.G. (2009). The rabbit biodistribution of a therapeutic dose of zoledronic acid labeled with Tc-99m. Appl Radiat Isot.
8 Smith M.R. (2008). Osteoclast targeted therapy for prostate cancer: bisphosphonates and beyond. Urol Oncol.